# 6-Deoxy-6-[^18^F]fluoro-D-fructose

Chemical name: | 6-Deoxy-6-[^18^F]fluoro-D-fructose
Abbreviated name: | 6-[^18^F]FDF
Synonym:
Agent Category: | Compound
Target: | Glucose transporters, ketohexokinase
Target Category: | Transporters, enzymes
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FDF)]

The phosphorylation of glucose, an initial and important step in cellular metabolism, is catalyzed by hexokinases (HKs) (1). There are four HKs in mammalian tissues. HKI, HKII, and HKIII have molecular weights of ~100,000 each. HKI is found mainly in the brain. HKII is insulin-sensitive and is found in adipose and muscle cells. HKIV, also known as glucokinase, has a molecular weight of 50,000 and is specific to the liver and pancreas. Most brain HK is bound to mitochondria, enabling coordination between glucose consumption and oxidation. Tumor cells are known to be highly glycolytic because of increased expression of glycolytic enzymes and HK activity (2), which is detected in tumors from patients with lung, gastrointestinal, and breast cancer. The HKs, by converting glucose to glucose-6-phosphate, help maintain the downhill gradient that results in the transport of glucose into cells through the facilitative glucose transporters (GLUT1-13) (3). GLUT4 and HKII are the major transporter and HK isoform in skeletal muscle, heart, and adipose tissue, wherein insulin promotes glucose utilization. HKIV is associated with GLUT2 in liver and pancreatic β cells.

2-Deoxy-D-glucose (2DG) was first developed to inhibit glucose utilization by cancer cells (4). HKs phosphorylate 2DG to 2-DG-6-phosphate, which inhibits phosphorylation of glucose. 2-[^18^F]Fluoro-2-deoxy-D-glucose ([^18^F]FDG) was later developed for molecular imaging studies (5). FDG is moved into cells by glucose transporters (GLUT1 and GLUT3) and is then phosphorylated by HK to FDG-6-phosphate. FDG-6-phosphate cannot be metabolized further in the glycolytic pathway and remains within the cells. Tumor cells do not contain a sufficient amount of glucose-6-phosphatase to reverse the phosphorylation. The elevated rates of glycolysis and glucose transport in many types of tumor cells and activated cells enhance the uptake of FDG in these cells relative to other normal cells. Positron emission tomography (PET) with [^18^F]FDG has been used to assess alterations in glucose metabolism in brain, cancer, cardiovascular diseases, Alzheimer’s disease and other central nervous system disorders, and infectious, autoimmune, and inflammatory diseases (6-11).

Overall, [^18^F]FDG PET showed 76%–89% sensitivity and 73%–80% specificity for the detection of primary breast cancer (12). Several clinical studies showed that 28%–47% of breast tumor samples were negative for GLUT1 (13, 14). The low or absent tumor expression of GLUT1 seems to account for the low sensitivity of [^18^F]FDG PET in detecting these breast tumors. High-affinity fructose transporter GLUT5 was found to be overexpressed in 37% of breast tumor samples (13). 6-Deoxy-6-fluoro-D-fructose (6-FDF) is a substrate for GLUT5, whereas FDG is not (15). Wuest et al. (16) have evaluated 6-deoxy-6-[^18^F]fluoro-D-fructose (6-[^18^F]FDF) as a PET tracer for imaging GLUT5 expression.

### Related Resource Links:

- Chapters in MICAD (Hexokinase (http://www.ncbi.nlm.nih.gov/books?term=(hexokinase%20OR%20hexokinases)%20AND%20micad%5Bbook%5D), glucose transporter (http://www.ncbi.nlm.nih.gov/books?term=glucose%20transporters%20%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Hexokinase (http://www.ncbi.nlm.nih.gov/gene?term=hexokinase%20human), Glut1 (http://www.ncbi.nlm.nih.gov/gene/6513), Glut5 (http://www.ncbi.nlm.nih.gov/gene/6518)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (Hexokinase (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=hexokinase%5BAll+Fields%5D), Glut1 (http://www.ncbi.nlm.nih.gov/omim/138140), Glut5 (http://www.ncbi.nlm.nih.gov/omim/138230))
- Clinical trials ([^18^F]FDG (http://www.clinicaltrials.gov/ct2/results?term=FDG))
- Drug information in FDA ([^18^F]FDG (http://google2.fda.gov/search?q=%5B18F%5DFDG&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=3&y=9))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FDF%20AND%20%22chemical%20synthesis%22%5BSubheading%5D)]

6-[^18^F]FDF was readily synthesized with standard ^18^F-fluorination of the triflate derivative with ([^18^F]KF/Kryptofix 2.2.2, 8 min at 85°C) and subsequent acid hydrolysis with 2N HCl (8 min at 110°C) in an automated module (16). Overall radiochemical yields were 25%–35%, with a radiochemical purity of >95%. The synthesis time was ~120 min, including high-performance liquid chromatography purification. The specific activity of 6-[^18^F]FDF was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FDF%20AND%20in%20vitro)]

Wuest et al. (16) showed that 6-[^18^F]FDF entered murine EMT-6 and human MCF-7 breast tumor cells in culture with 30 ± 4% (n = 9) and 12 ± 1% (n = 7) incubation dose/mg protein after 60 min of incubation, respectively. In comparison, [^18^F]FDG accumulation in these two tumor cells was >10-fold higher. 6-FDF exhibited a 9-fold higher potency than D-fructose to inhibit 6-[^18^F]FDF accumulation in EMT-6 cells, whereas D-glucose showed no inhibition. 6-[^18^F]FDF was not retained in the tumor cells as >80% of radioactivity was found in the fresh medium after 60 min incubation. Approximately 65%–75% intact 6-[^18^F]FDF was found in the tumor cells. On the other hand, most of the radioactivity from [^18^F]FDG was trapped inside the cells. 6-[^18^F]FDF was rapidly phosphorylated by the human recombinant ketohexokinase but not by human recombinant HKII in cell-free enzyme assays.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FDF%20AND%20rodentia%20NOT%20in%20vitro)]

6-[^18^F]FDF accumulated rapidly in kidneys, heart, liver, spleen, gallbladder, lung, and intestines of normal mice (n = 3/group) at 5 min after injection, followed by rapid clearance (16). On the other hand, the moderate accumulation of the tracer in the brain remained relatively constant during the 2-h experiment. Radioactivity in the bone increased with time, indicating radiodefluorination of 6-[^18^F]FDF. Ex vivo biodistribution studies were also performed in mice (n = 3/group) bearing EMT-6 tumors. The organ with the highest accumulation was the kidney (12.3% injected dose/gram (ID/g)) at 5 min after injection. Tumor accumulation was 3.7% ID/g, 3.5% ID/g, and 1.8% ID/g at 5, 30, and 120 min after injection, respectively. Blood and muscle radioactivity levels were 1.5% ID/g and 0.9% ID/g at 120 min, respectively. Plasma contained 24% and 10% intact 6-[^18^F]FDF at 5 min and 60 min after injection with one more polar radiometabolite and one more lipophilic radiometabolite. No blocking study was performed.

PET imaging studies were performed in mice bearing EMT-6 tumors (n = 3/group) and nude mice bearing MCF-7 tumors (n = 3/group) with 6-[^18^F]FDF and [^18^F]FDG at 15 min and 120 min after injection (16). The EMT-6 tumors were visualized with both tracers at both time points. Both tracer accumulations in the MCF-7 tumors were less visible than in the EMT-6 tumors. 6-[^18^F]FDF reached a maximum standard uptake value (SUV) of 1.23 ± 0.09 at 10–15 min and decreased to 0.54 ± 0.06 at 120 min. On the other hand, [^18^F]FDG increased consistently over 120 min, reaching a maximum SUV of 1.80 ± 0.25 at 120 min. Maximum SUV values of both tracers (~0.75) in MCF-7 tumors were similar at 10–15 min after injection but were lower than those of EMT-6 tumors. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FDF%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FDF%20AND%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FDF%20AND%20humans)]

No publication is currently available.

## References

1 Smith T.A. (2000). Mammalian hexokinases and their abnormal expression in cancer. Br J Biomed Sci.
2 Suolinna E.M., Haaparanta M., Paul R., Harkonen P., Solin O., Sipila H. (1986). Metabolism of 2-[18F]fluoro-2-deoxyglucose in tumor-bearing rats: chromatographic and enzymatic studies. Int J Rad Appl Instrum B.
3 Avril N. (2004). GLUT1 expression in tissue and (18)F-FDG uptake. J Nucl Med.
4 Laszlo J., Humphreys S.R., Goldin A. (1960). Effects of glucose analogues (2-deoxy-D-glucose, 2-deoxy-D-galactose) on experimental tumors. J Natl Cancer Inst.
5 Fowler J.S., Ido T. (2002). Initial and subsequent approach for the synthesis of 18FDG. Semin Nucl Med.
6 Phelps M.E. (2000). PET: the merging of biology and imaging into molecular imaging. J Nucl Med.
7 Phelps M.E., Mazziotta J.C. (1985). Positron emission tomography: human brain function and biochemistry. Science.
8 Phelps M.E., Mazziotta J.C., Huang S.C. (1982). Study of cerebral function with positron computed tomography. J Cereb Blood Flow Metab.
9 Rohren E.M., Turkington T.G., Coleman R.E. (2004). Clinical applications of PET in oncology. Radiology.
10 Sokoloff L. (1985). Basic principles in imaging of regional cerebral metabolic rates. Res Publ Assoc Res Nerv Ment Dis.
11 Spence A.M., Mankoff D.A., Muzi M. (2003). Positron emission tomography imaging of brain tumors. Neuroimaging Clin N Am.
12 Younes M., Brown R.W., Mody D.R., Fernandez L., Laucirica R. (1995). GLUT1 expression in human breast carcinoma: correlation with known prognostic markers. Anticancer Res.
13 Godoy A., Ulloa V., Rodriguez F., Reinicke K., Yanez A.J., Garcia Mde L., Medina R.A., Carrasco M., Barberis S., Castro T., Martinez F., Koch X., Vera J.C., Poblete M.T., Figueroa C.D., Peruzzo B., Perez F., Nualart F. (2006). Differential subcellular distribution of glucose transporters GLUT1-6 and GLUT9 in human cancer: ultrastructural localization of GLUT1 and GLUT5 in breast tumor tissues. J Cell Physiol.
14 Zamora-Leon S.P., Golde D.W., Concha, Rivas C.I., Delgado-Lopez F, Baselga J, Nualart F, Vera J.C. (1996). Expression of the fructose transporter GLUT5 in human breast cancer. Proc Natl Acad Sci U S A.
15 Chan K.K., Chan J.Y., Chung K.K., Fung K.P. (2004). Inhibition of cell proliferation in human breast tumor cells by antisense oligonucleotides against facilitative glucose transporter 5. J Cell Biochem.
16 Wuest M., Trayner B.J., Grant T.N., Jans H.S., Mercer J.R., Murray D., West F.G., McEwan A.J., Wuest F., Cheeseman C.I. (2011). Radiopharmacological evaluation of 6-deoxy-6-[18F]fluoro-D-fructose as a radiotracer for PET imaging of GLUT5 in breast cancer. Nucl Med Biol.